# ^99m^Tc-[Ac-CCEHdFRWCKPV-NH_2_]

Chemical name: | ^99m^Tc-[Ac-CCEHdFRWCKPV-NH_2_]
Abbreviated name: | ^99m^Tc-CCMSH
Synonym: | ^99m^Tc-cyclic α-MSH, ^99m^Tc-labeled cyclic α-melanocyte−stimulating hormone peptides, ^99m^Tc-[Cys^3,4,10^,D-Phe^7^]α-MSH_3-13_, ^99m^Tc-[Acetyl-Cys-Cys-Glu-His-dPhe-Arg-Trp-Cys-Lys-Pro-Val-NH_2_]
Agent Category: | Peptide
Target: | Melanocortin-1 (MC-1) receptor
Target Category: | Peptide-receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | ^99m^Tc-[Ac-CCEHdFRWCKPV-NH_2_] structure. The ^99m^Tc coordination configuration has not been confirmed by experiments. Click on sid:49693200 (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?sid=49693200&loc=ec_rcs) for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-%20CCMSH)]

^99m^Tc-[Ac-CCEHdFRWCKPV-NH_2_] (^99m^Tc-CCMSH) is a radioligand that has been developed as a single-photon emission computed tomography (SPECT) imaging probe for primary and metastatic melanoma (1, 2). ^99m^Tc-CCMSH is an α-melanocyte−stimulating hormone (MSH) peptide labeled with ^99m^Tc, a gamma emitter with a physical half-life (t_½_) of 6.02 h.

Malignant melanoma is the sixth most common cancer in the United States (3). Early diagnosis and prompt surgical removal make up the best approach for a possible cure (4). The melanocortin (MC) system is the best characterized neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (5). Most cutaneous cell types express MC receptors, proopiomelanocortin (POMC), and prohormone convertases, and these cell types also release MCs. Five MC receptors (MC-1 to MC-5) have been cloned and characterized as receptors that belong to the G-protein−coupled receptor superfamily. MSHs (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_) is a peptide composed of 13 amino acids and is the most potent, naturally occurring, melanotropic peptide (6). The biological effects of α-MSH are mediated via MC receptors.

Although positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (7, 8). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC-1 receptors that are overexpressed on human and mouse melanoma cells (7, 9-12). Some studies have successfully used 1,4,7,10-tetraazacyclodecane-N,N',N'',N'''-tetraacetic acid (DOTA) coupled to the α-MSH peptide analogs for radiolabeling. These α-MSH derivatives (DOTA-α-MSH) can be labeled with a variety of radionuclides (7). To improve the in vivo pharmacokinetics of these radiolabeled peptides, a number of different α-MSH analogs have been designed (13, 14). Froidevaux et al. (13) showed that the kidney uptake of DOTA-NAPamide, a short linear DOTA−α-MSH analog, could be considerably reduced by neutralizing the charge of the Lys^11^ residue. Giblin et al. (2) used metal cyclization to design a new class of α-MSH peptide analogs that are resistant to chemical and proteolytic degradation in vivo, and their study showed that ^99m^Tc-CCMSH complex had potential melanoma-imaging properties. Chen et al. (1) reported that ^99m^Tc-CCMSH analogs, cyclized through site-specific coordination of ^99m^TcO, showed excellent tumor uptake and retention properties in mice bearing B16/F1 murine melanomas.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-%20CCMSH%20AND%20synthesis)]

The CCMSH peptide was synthesized by using the standard fluorenylmethoxycarbonyl/2(1H-benzotriazol-1-yl)-1,1,3,3,tetramethyluronium hexafluorophosphate solid-phase peptide synthesis chemistry on amide resin (1, 2). A solid-phase peptide synthesizer was used. The peptide was acetylated by activating glacial acetic acid with 2(1H-benzotriazol-1-yl)-1,1,3,3,tetramethyluronium hexafluorophosphate after deprotecting the NH_2_-terminal residue. The peptide was deprotected and cleaved from the resin by using a mixture of trifluoroacetic acid, thioanisol, ethanedithiol, and water at room temperature for 2 h. The peptide was then purified by high-performance liquid chromatography (HPLC), and the identity was confirmed by fast atom bombardment mass spectrometry. The molecular weight of CCMSH was determined to be 1,448 (calculated molecular weight = 1,447). The ^99m^Tc radiolabeling was prepared via a glucoheptonate transchelation reaction (1). In this procedure, stannous chloride (SnCl_2_) was used as a reducing agent and glucoheptonate was used as a transfer ligand. Briefly, 10 μg of the peptide were added to the mixture of SnCl_2_, ^99m^Tc-pertechnetate, and glucoheptonate after the pH of the mixture was adjusted to 9. The mixture was incubated at 75ºC for 30 min. The final ^99m^Tc-CCMSH product was purified by HPLC. The identity of ^99m^Tc-CCMSH was confirmed by both mass spectrometry and HPLC analysis. The radiochemical stability was evaluated in phosphate-buffered saline (PBS; pH 7.4). Over a 24-h period of incubation at 25ºC in PBS, only radiolabeled peptide and no detectable free radioactivity was detected by HPLC analysis (1). The specific activity and radiochemical purity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-%20CCMSH%20AND%20in%20vitro)]

Giblin et al. (2) performed in vitro quantitative receptor-binding assays of unlabeled CCMSH on B16/F1 murine melanoma cells. The inhibition constant (K_i_) was determined to be 7.6 × 10−^9^ M.

Chen et al. (1) performed receptor binding affinity, internalization, and cellular retention assays of ^99m^Tc-CCMSH on B16/F1 murine melanoma cells. A B_max_ of 5.812 fmol/0.5 million cells (7,000 α-MSH receptors/cell) were determined. About 4% cell binding was found after 3 h of incubation. As early as 5 min after incubation, ~70% of the receptor-bound radioligand was internalized. This percentage of internalized radioactivity did not significantly change over the incubation period. When testing for cellular retention, ~36% of the internalized radioactivity was released from the cells during a 4-h incubation at 37ºC. Analysis using a C-18 Sep-Pak column showed that the majority of the radioactivity released from the cells consisted of low molecular weight forms.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-%20CCMSH%20AND%20rodentia)]

Biodistribution and gamma imaging studies with ^99m^Tc-CCMSH were conducted in normal mice and mice bearing the B16/F1 murine melanoma (2). Each mouse received 74–111 MBq (2–3 mCi) of ^99m^Tc-CCMSH by i.v. administration. ^99m^Tc-CCMSH radioactivity was rapidly cleared and excreted by the kidneys in the healthy mice. In melanoma-bearing mice, ^99m^Tc-CCMSH radioactivity accumulated rapidly in the tumor. The radioactivity levels in the tumor (n = 5), shown as percentage injected dose per g (% ID/g) at various time points, were 10.74 ± 1.61 (0.5 h), 10.88 ± 0.54 (1 h), 9.51 ± 1.97 (4 h), and 1.38 ± 0.36 (24 h). The tumor/blood ratios were 3.12 (0.5 h), 6.80 (1 h), and 15.34 (4 h). The activity was cleared rapidly from the tumor-bearing animals with 74.84 ± 2.53% ID/g in the urine at 1 h. Other major organ radioactivity levels (% ID/g) at 1 h were 22.60 ± 2.70 (kidneys), 2.34 ± 2.19 (liver), 1.39 ± 0.20 (lung), 0.53 ± 0.17 (heart), 1.07 ± 0.26 (spleen), and 0.90 ± 0.10 (muscle). The radioactivity in the stomach (% ID/g) was 0.47 ± 0.10 at 1 h. Coinjection of 30 mg lysine appeared to reduce kidney radioactivity uptake by 48%, 55%, and 70% at 0.5, 1, and 4 h after injection, respectively (1). With injection of 1 mg of NDP ([NIe^4^,D-Phe^7^] αMSH), a high-affinity unlabeled α-MSH analog, 30 min before ^99m^Tc-CCMSH injection, the tumor radioactivity was reduced from an average of 8.5% ID to 0.82% ID at 30 min (2). A tumor imaging study with a dose of 925 MBq (25 mCi) in a mouse bearing a 400-mg melanoma showed tumor visualization and significant tumor radioactivity accumulation at 30 min. The kidneys and bladder also showed radioactivity uptake. Another imaging study with a dose of 3.7 MBq (0.1 mCi) showed that the tumor was visualized after 1 h, and the tumor activity was extremely high at 8 h (1). The bladder activity was very high at 1 h, and the background in the normal tissues was low after the bladder contents were voided at 8 h.

The same group of researchers performed biodistribution studies of ^99m^Tc-CCMSH in SCID mice bearing TXM-13JQ human melanomas (1). The TXM-13JQ human melanoma had a B_max_ value of 5.812 fmol/0.5 million cells (7,000 α-MSH receptors/cell). Each mouse received 0.925 MBq (0.025 mCi) ^99m^Tc-CCMSH for the studies. The biodistribution pattern of ^99m^Tc-CCMSH radioactivity in normal tissues was similar to those of mice bearing B16/F1 murine melanomas. The radioactivity levels (% ID/g) in the tumor (n = 5) were 3.08 ± 0.58 (0.5 h), 3.26 ± 0.77 (1 h), 2.22 ± 0.25 (4 h), and 0.48 ± 0.12 (24 h). The tumor/blood ratios were 1.15 (0.5 h), 2.03 (1 h), 5.82 (4 h), and 3.31 (24 h). The tumor/muscle ratios were 7.89 (0.5 h), 11.55 (1 h), 38.71 (4 h), and 27.50 (24 h). Coinjection of 30 mg lysine decreased both the kidney and blood radioactivity levels. As a result, the tumor/blood ratios were improved to 1.44 (0.5 h), 4.11 (1 h), 11.52 (4 h), and 4.56 (24 h). The tumor/muscle ratios were improved to 6.17 (0.5 h), 19.14 (1 h), 50.90 (4 h), and 37.14 (24 h).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-%20CCMSH%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-%20CCMSH%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-%20CCMSH%20AND%20human)]

No publication is currently available.

## References

1 Chen J., Cheng Z., Hoffman T.J., Jurisson S.S., Quinn T.P. (2000). Melanoma-targeting properties of (99m)technetium-labeled cyclic alpha-melanocyte-stimulating hormone peptide analogues. Cancer Res.
2 Giblin M.F., Wang N., Hoffman T.J., Jurisson S.S., Quinn T.P. (1998). Design and characterization of alpha-melanotropin peptide analogs cyclized through rhenium and technetium metal coordination. Proc Natl Acad Sci U S A.
3 Miao Y., Benwell K., Quinn T.P. (2007). 99mTc- and 111In-labeled alpha-melanocyte-stimulating hormone peptides as imaging probes for primary and pulmonary metastatic melanoma detection. J Nucl Med.
4 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
5 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
6 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
7 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
8 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
9 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
10 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
11 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
12 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
13 Froidevaux S., Calame-Christe M., Tanner H., Eberle A.N. (2005). Melanoma targeting with DOTA-alpha-melanocyte-stimulating hormone analogs: structural parameters affecting tumor uptake and kidney uptake. J Nucl Med.
14 Miao Y., Owen N.K., Whitener D., Gallazzi F., Hoffman T.J., Quinn T.P. (2002). In vivo evaluation of 188Re-labeled alpha-melanocyte stimulating hormone peptide analogs for melanoma therapy. Int J Cancer.